# CellVue Maroon–labeled saposin C-dioleylphosphatidylserine nanovesicles

Chemical name: | CellVue Maroon–labeled saposin C-dioleylphosphatidylserine nanovesicles
Abbreviated name: | CVM-SapC-DOPS
Synonym:
Agent Category: | Nanoparticles
Target: | Phospholipids
Target Category: | Lipids
Method of detection: | Optical imaging
Source of signal / contrast: | CellVue Maroon
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging)]

The CellVue Maroon (CVM)–labeled saposin C (SapC)-dioleylphosphatidylserine (DOPS) nanovesicle, abbreviated as CVM-SapC-DOPS, is an imaging agent developed by Qi et al. and Kaimal et al. for phospholipid (PS)-targeted optical imaging (1, 2).

Saposins are a group of water-soluble lysosomal glycoproteins (SapA, SapB, SapC, and SapD) with molecular weights of 8–11 kDa (1-3). They are generated by the proteolytic processing of the common precursor prosaposin. Saposins localize primarily in the lysosomes and are required for the catabolism of glycosphingolipids (4, 5). The four saposins have a high degree of structural similarity and share lipid-binding and membrane-perturbing properties; however, they behave differently and exhibit different specificities (1, 3). SapC is the second saposin to be discovered, and it binds to membranes in a pH-controlled manner (6). SapC can directly activate enzymes and stimulate the hydrolysis of glycocerebroside and galactocerebroside (7). Deficiency of SapC leads to an abnormal juvenile form of Gaucher disease with accumulation of glucosylceramide in various organs, including the brain (5).

SapC preferentially interacts with unsaturated, negatively charged PS such as DOPS at acidic pH (6, 8). PS is present in all cells and constitutes ~2%–10% of total cellular lipids. In normal tissues, PS is localized in the cell membrane leaflets that face the cytosol. However, in pathological conditions such as tumors, PS translocates to the outer leaflet of the plasma membrane, where it activates and participates in various cellular processes, including apoptosis and necrosis (5, 9). Phagocytes in healthy tissues rapidly and efficiently remove the PS-expressing cells and cell remnants, but these PS-expressing cells and cell remnants accumulate in diseased tissues as a result of the activation of the cell death process and the insufficient clearance of cells expressing PS externally (9).

Because tumors express abundant PS on the cell surface and have a lower extracellular pH (pH ~6) than normal tissues (pH ~7), the SapC-PS interaction provides a valuable system for targeted tumor imaging and therapy (4, 9, 10). Qi et al. developed a SapC-DOPS nanovesicle system that induced apoptosis of tumor cells in vitro and inhibited growth of neuroblastomas and malignant peripheral nerve sheath tumors in animal models (1). Both fluorescently labeled SapC-DOPS (CVM-SapC-DOPS) and iron oxide particle–coupled SapC-DOPS (SapC-DOPS-IO) have been shown to preferentially accumulate in tumor xenografts (1, 2). These studies indicate that SapC-DOPS nanovesicles are promising as a new and robust theranostic agent for cancer-selective detection, visualization, and therapy. This chapter summarizes the data obtained with CVM-SapC-DOPS. The data obtained with SapC-DOPS-IO (http://www.ncbi.nlm.nih.gov/books/NBK5330/) are summarized in another chapter in MICAD.

### Related Resource Links:

- Protein information for saposin C (http://www.ncbi.nlm.nih.gov/protein/?term=saposin+C)
- Protein information for prosaposin (http://www.ncbi.nlm.nih.gov/protein?term=prosaposin)
- Saposin-related compounds in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=saposin)
- Saposin-related articles in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=saposin)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging%20and%20therapy)]

Qi et al. described the synthesis of CVM-SapC-DOPS nanovesicles in detail (1). Briefly, recombinant human SapC was expressed in Escherichia coli cells. Pure SapC was then mixed with lipids in acid buffer (pH 5). The protein–lipid mixture was gently sonicated and ultracentrifuged to produce SapC-DOPS nanovesicles in pellet form. No SapC was detected in the supernatant fraction, indicating a very high loading/coupling efficiency. The sonicated SapC-DOPS complexes contained monodispersed, unilamellar vesicles with a mean diameter of ~190 nm.

CVM-SapC-DOPS nanovesicles were generated by mixing CVM with SapC-DOPS (1, 2). CVM is a commercially available lipophilic fluorescent probe. CVM-SapC-DOPS nanovesicles were separated from free dye with a Sephadex G25 column. The CVM-SapC-DOPS nanovesicles had an excitation maximum at 653 nm and an emission maximum at 677 nm. SapC-DOPS nanovesicles were spherical, and the addition of CVM did not alter the nanovesicle shape. The molar ratio of CVM/SapC/DOPS was 0.4:1:2.6 in the CVM-SapC-DOPS nanovesicles.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging%20and%20therapy)]

Qi et al. tested the in vitro internalization of CVM-SapC-DOPS after incubation with human neuroblastoma cells (CHLA-20) for 12 h (1). Microscopy showed a strong intracellular fluorescent signal, indicating that the agent could be incorporated into tumor cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging%20and%20therapy)]

Qi et al. used real-time fluorescence imaging to analyze the in vivo biodistribution of CVM-SapC-DOPS in one mouse bearing a neuroblastoma xenograft (1). Control mice were administered an uncoupled SapC and CVM-DOPS complex or CVM-DOPS alone (n = 1 mouse/agent). At the early time points (0.5 h and 5 h) after agent injection, fluorescent signal was detected in both tumor and nontumor tissues (likely liver). At 12 h after injection, the fluorescent signal at the tumor site was observed in the mice injected with CVM-SapC-DOPS or with the uncoupled SapC and CVM-DOPS complex. Animals injected with CVM-DOPS alone showed minimal fluorescence distribution at the early time points, which was absent by 12 hours after injection. By 24 h, the fluorescence in tumors was detected only in animals injected with CVM-SapC-DOPS, and this signal was detectable for at least 48 h.

In vivo biodistribution of SapC was studied with SapC labeled with Alexa Flour 660 instead of CVM because CVM is a lipophilic fluorescent dye (1). No fluorescent signal was detected in tumor sites after injection of Alexa Flour 660–labeled SapC alone, suggesting that SapC alone has no readily detectable tumor-targeting property.

Immunohistochemistry of the tumor sections revealed a strong CVM signal in the tumor cells and vessels from animals treated with CVM-SapC-DOPS but not in control tumors (1). SapC from the CVM-SapC-DOPS was further confirmed to be located in tumor cells with specific antibodies and not within adjacent stromal tissues. Fluorescent signal of CVM-SapC-DOPS vesicles was also detected in the liver and spleen, but this signal decreased to the point of being undetectable by 24 h after injection.

Qi et al further estimated the tumor-targeting efficiency of CVM-SapC-DOPS (1). At 24 h after intravenous injection, tumor-bearing mice showed a tumor uptake efficiency of 43% as measured by in vivo quantification of the fluorescent signal intensity.

Kaimal et al. conducted optical imaging with CVM-SapC-DOPS in mice bearing human pancreatic (MiaPaCa-2) xenografts, neuroblastoma xenografts, and murine rhabdomyosarcoma allografts (n = 1 mouse per tumor type) (2). In mice with pancreatic tumor xenografts, the fluorescent signal of CVM-SapC-DOPS was detected in both tumor and nontumor tissues (likely liver) at 2 h after injection, but this signal increased significantly in tumor sites and decreased in nontumor tissues at the time points from 2 h to 24 h. Tumor-homing fluorescence remained for at least 100 h. Images of mice with human neuroblastoma xenografts showed tumor fluorescence in a mouse injected with CVM-SapC-DOPS (n = 1) not in a mouse injected with uncoupled SapC and CMV-DOPS (n = 1) or CVM-DOPS alone (n = 1). The tumor-selective behavior of CVM-SapC-DOPS was further confirmed with optical imaging in a mouse with a rhabdomyosarcoma allograft (detailed data not shown) (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Qi X., Chu Z., Mahller Y.Y., Stringer K.F., Witte D.P., Cripe T.P. (2009). Cancer-selective targeting and cytotoxicity by liposomal-coupled lysosomal saposin C protein. Clin Cancer Res.
2 Kaimal, V., Z. Chu, Y.Y. Mahller, B. Papahadjopoulos-Sternberg, T.P. Cripe, S.K. Holland, and X. Qi, Saposin C Coupled Lipid Nanovesicles Enable Cancer-Selective Optical and Magnetic Resonance Imaging. Mol Imaging Biol, 2010
3 Rossmann M., Schultz-Heienbrok R., Behlke J., Remmel N., Alings C., Sandhoff K., Saenger W., Maier T. (2008). Crystal structures of human saposins C andD: implications for lipid recognition and membrane interactions. Structure.
4 Wang Y., Grabowski G.A., Qi X. (2003). Phospholipid vesicle fusion induced by saposin C. Arch Biochem Biophys.
5 Atrian S., Lopez-Vinas E., Gomez-Puertas P., Chabas A., Vilageliu L., Grinberg D. (2008). An evolutionary and structure-based docking model for glucocerebrosidase-saposin C and glucocerebrosidase-substrate interactions - relevance for Gaucher disease. Proteins.
6 Abu-Baker S., Qi X., Newstadt J., Lorigan G.A. (2005). Structural changes in a binary mixed phospholipid bilayer of DOPG and DOPS upon saposin C interaction at acidic pH utilizing 31P and 2H solid-state NMR spectroscopy. Biochim Biophys Acta.
7 Nieh M.P., Pencer J., Katsaras J., Qi X. (2006). Spontaneously forming ellipsoidal phospholipid unilamellar vesicles and their interactions with helical domains of saposin C. Langmuir.
8 Abu-Baker S., Qi X., Lorigan G.A. (2007). Investigating the interaction of saposin C with POPS and POPC phospholipids: a solid-state NMR spectroscopic study. Biophys J.
9 Schutters K., Reutelingsperger C. (2010). Phosphatidylserine targeting for diagnosis and treatment of human diseases. Apoptosis.
10 Zhang X., Lin Y., Gillies R.J. (2010). Tumor pH and its measurement. J Nucl Med.